# IR-786 perchlorate

Chemical name: | IR-786 perchlorate
Abbreviated name: | IR-786
Synonym: | 2-(2-[2-Chloro-3-([1,3-dihydro-1,3,3-trimethyl-2H-indol-2-ylidene]ethylidene)-1-cyclohexen-1-yl]ethenyl)-1,3,3-trimethylindolium perchlorate
Agent category: | Compound
Target: | Mitochondria and endoplasmic reticulum
Target category: | Lipophilic cation
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal\contrast: | IR-786
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IR-786%5BAll%20Fields%5D)]

Optical fluorescence imaging is increasingly used to obtain biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when visible light (350-700 nm) absorbing fluorophores are used. Near-infrared (NIR) fluorescence (700-900 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging.

IR-786 perchlorate (IR-786) is a heptamethine indocyanine-type NIR fluorophore with peak absorption in the 760-780-nm range and peak excitation emission in the 795-815-nm range. It provides a quantum yield of 3.3%. IR-786 is a lipophilic cation, localized to mitochondria at low concentrations and to endoplasmic reticulum (ER) at high concentrations (3). It has a molecular weight of 584. IR-786 proves to be a useful agent in myocardial and brown adipose tissue (BAT) perfusion (4). In mice, two large, lobulated masses of brown fat tissue are found on the dorsal side of the thorax. BAT is located in smaller masses around the aorta and in the hilus of the kidney. BAT is richly vascularised and has numerous unmyelinated nerves, which provide sympathetic stimulation from the hypothalamus to the adipocytes (5). Brown adipocytes express mitochondrial uncoupling proteins, which give the cell's mitochondria an ability to uncouple oxidative phosphorylation and utilize substrates to generate heat rather than ATP (5-8). NIR fluorescence dyes with N-hydoxysuccinimide ester can be conjugated to antibodies and low-molecular weight ligands (9).

### Related Resource Links:

- Chapters in MICAD (IR-786 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=IR-786+AND+micad%5Bbook%5D))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IR-786%5BAll%20Fields%5D%20AND%20%28%22chemical%20synthesis%22%5BSubheading%5D%20OR%20synthesis%5BAll%20Fields%5D%29)]

IR-786 perchlorate is commercially available (LI-COR, Lincoln, NE).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IR-786%5BAll%20Fields%5D%20AND%20in%20vitro)]

IR-786 uptake into rat neonatal cardiomyocytes, human T24 bladder carcinoma, and mouse MBT-2 bladder carcinoma was rapid with plateau levels within 30 min (4). These cells incorporated 2.2-6.1 fmol of IR-786 per cell when incubated with 10 μM dye. IR-786 accumulated exclusively in mitochondria of these cells at or below extracellular concentrations of 0.25, 1, and 0.25 μM, respectively, and in both mitochondria and ER at above the threshold concentrations. Pretreatment of cells with 10 μM FCPP, which dissipates the mitochondrial membrane potential abolished mitochondrial uptake of both IR-876 and rhodamine 123. Both the dyes were now localized exclusively in the ER. The cells were visualized directly using NIR fluorescence microscopy. The mitochondria were found to be structurally intact by staining with a mitochondria-specific antibody.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IR-786%5BAll%20Fields%5D%20AND%20rodentia)]

Rats were injected intravenously with 50 nmol of IR-786 (3). Peak serum concentration of 0.13 μM was reached within 1 min. A peak uptake of 1.7% injected dose (about 0.6 μM) was observed in the explanted heart at 1 min. NIR fluorescence reflectance imaging showed peak emission fluorescence intensity from the exposed heart at 1 min, returning to baseline within 1 h. When left anterior descending coronary artery occlusion was introduced for 5 min, the myocardium distal to the occlusion had a 4-fold decrease in fluorescence signal compared with the perfused myocardium. When the occlusion was removed, IR-786 fluorescence was homogeneous in the heart within 1 min. Prolonged ischemia (30-min occlusion) showed a large area with no IR-786 fluorescence. At 24 h after occlusion, the beating heart was imaged again. IR-786 revealed a 1.6-fold increase in perfusion from dilated arteries, showing a 1.4-mm-wide, crescent-shaped, infarcted band. The infarcted area was confirmed with 2,3,5-triphenyltetrazolium chloride staining and by tissue sectioning as 49.5% of the area at risk and 47.1% as measured by IR-786 fluorescence. IR-786 can be used to finely map myocardial blood flow, perfusion, and infarction.

Nude mice were injected intravenously with 1 nmol of IR-786, and various organs were removed and measured fluorometrically (4). An avid accumulation of IR-786 was found in the lungs within 1 min, decreasing over 24 h. The liver and spleen uptake increased with time, peaking at 1 h. The blood concentration remained low. Negligible uptake was seen in the muscle, kidneys, and brain. The other areas with significant uptake were the heart and thorax BAT. β3-Adrenergic (Cl 316,243) and cold (4ºC) stimulation of mice increased uptake in thorax BAT, as imaged by NIR fluorescence reflectance imaging. The β3-adrenergic antagonist, propanolol, blocked the cold stimulation-induced uptake in BAT. BAT perfusion fluorescence intensity of IR-786 was similar in nude mice with or without their skin removed. Using homozygous deletion of uncoupling proteins 1 and 2, these mice had a higher baseline perfusion of BAT but a similar maximal response to Cl 316,243. BAT perfusion can be measured non-invasively, and pharmacological modulators of thermogenesis can be screened in living animals using NIR fluorescence.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IR-786%5BAll%20Fields%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29%20)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IR-786%5BAll%20Fields%5D%20AND%20primate%20NOT%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IR-786%5BAll%20Fields%5D%20AND%20human)]

No publication is currently available.

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Nakayama A., del Monte F., Hajjar R.J., Frangioni J.V. (2002). Functional near-infrared fluorescence imaging for cardiac surgery and targeted gene therapy. Mol Imaging.
4 Nakayama A., Bianco A.C., Zhang C.Y., Lowell B.B., Frangioni J.V. (2003). Quantitation of brown adipose tissue perfusion in transgenic mice using near-infrared fluorescence imaging. Mol Imaging.
5 Morrison S.F. (2004). Central pathways controlling brown adipose tissue thermogenesis. News Physiol Sci.
6 Cannon B., Nedergaard J. (2004). Brown adipose tissue: function and physiological significance. Physiol Rev.
7 Klaus S. (2004). Adipose tissue as a regulator of energy balance. Curr Drug Targets.
8 Sell H., Deshaies Y., Richard D. (2004). The brown adipocyte: update on its metabolic role. Int J Biochem Cell Biol.
9 Zaheer A., Wheat T.E., Frangioni J.V. (2002). IRDye78 conjugates for near-infrared fluorescence imaging. Mol Imaging.